# [^18^F]Fluoroetanidazole

Chemical name: | N-(2-([^18^F]Fluoroethyl)-2(2-nitroimidazol-1-yl)-acetamide
Abbreviated name: | [^18^F]FETA
Synonym: | [^18^F]Fluoroetanidazole
Agent Category: | Compound
Target: | Hypoxic cells (macromolecules)
Target Category: | Intracellular reduction and binding
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoroetanidazole)]

Hypoxia in malignant tumors is thought to be a major factor limiting the efficacy of chemotherapy and radiotherapy, and its accurate diagnosis is considered a very important and urgent problem to address. This has led to the search and development of hypoxia-targeted imaging techniques and non-invasive markers of tumor hypoxia. Among these, [^18^F]-labeled nitroimidazoles, used in conjunction with positron emission tomography (PET), offer an alternative to the Eppendorf (oxygen) electrode method because they are less invasive and less prone to sampling errors.

During initial development of nitroimidazoles for in vivo imaging, radiohalogenated derivatives of misonidazole, such as fluoromisonidazole ([^18^F]FMISO), were used, some of which have been used in patients. The two main problems with [^18^F]FMISO are: 1) its relatively low concentration within the lesion; and 2) the need to wait several hours to allow clearance of the agent from the normoxic background tissue (contrast between lesion and background is typically <2:1 at about 90 min after injection). This combination of circumstances makes successful evaluation of hypoxic lesions a challenge, even with high-resolution positron emission tomography (PET).

Fluoroetanidazole ([^18^F]FETA), a fluorinated analog of etanidazole, is being investigated as a possible candidate for PET imaging of tumor hypoxia. Thus far, results from comparative studies between [^18^F]FETA and [^18^F]FMISO (1) have shown similar oxygen-dependent binding for both tracers, when compared in vitro on the same cell lines. In vivo, the two tracers displayed a similar retention in tumors at 4 h after injection, but fewer metabolites were found in plasma and urine for [^18^F]FETA, which might offer some advantages for in vivo imaging (2).

The oxygen-dependent metabolism of nitroimidazoles is an intracellular process consisting of a series of one-electron reductions. The nitro-radical anion produced in the first reduction step is very reactive toward oxygen, leaving no substrate for the second step of the reduction process. In contrast, an environment of low oxygen concentration induces further reductive reactions that ultimately lead to the formation of either reactive products that are able to covalently bind to cell components or charged species that diffuse slowly out of the tissues (3). The reactive products observed during this multi-step process include nitroso (2e-), hydroxylamine (4e-), and amine (6e-) derivatives. When the fragmentation of the imidazole ring occurs, reactive portions of the molecule, such as glyoxal, bind to macromolecular components of cells in tissues and tumors (4).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoroetanidazole%20AND%20synthesis)]

[^18^F]FETA can be synthesized by an active ester coupling reaction between the 2,3,5,6-tetrafluorophenyl ester of 2-nitroimidazole acetic acid and [^18^F]fluoroethylamine. [^18^F]Fluoroethylamine is prepared from N-[2-(toluene-4-sulfonyloxy)-ethyl]-phthalimide and [^18^F]fluoride. The reaction time of the total procedure is about 90 min, and the radiochemical yield (uncorrected) is about 25% (5).

Attempts have been made to synthesize [^18^F]FETA by fluorination of a sulfonate ester of etanidazole (6) and fluoroethylation of the amide (7), but these attempts were reported to be unsuccessful (5).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoroetanidazole%20AND%20in%20vitro)]

In vitro studies of [^18^F]FETA uptake in air versus nitrogen in RIF-1 cells were reported by Barthel et al. (2). In those experiments, cells were harvested at 0, 15, 30, 45, 60, 90, and 120 min after injection of the radiotracer (80-100 µCi (2.96-3.7 MBq)), and the percentage of bound radioactivity was calculated as bound radioactivity in 10^6^ cells × 100/total radioactivity.

The percentage of bound radioactivity under normoxic conditions remained low (about 2 × 10−^3^% per 10^6^ cells). In contrast, a rapid time-dependent linear increase was observed under hypoxic conditions (reaching about 13 × 10−^3^% per 10^6^ cells at 120 min). [^18^F]FETA uptake by hypoxic RIF-1 cells became significant at 60 min and showed 3.0- and 4.3-fold increases as compared with normoxic cells at 60 and 120 min, respectively. Those results appeared consistent with the presence of a 2-nitroimidazole moiety with redox potentials (E1/7) within the range of 380 to −390 mV (8).

In the study reported by Rasey et al. (1), the oxygen dependency of [^18^F]FETA binding to cells was investigated on the four cultured rodent cell lines V79, 36B10, EMT6, and RIF-1. Results showed that O_2_ levels of 600-1300 ppm inhibited binding by 50%, relative to uptake under anoxic conditions (<10 ppm). Those values were not statistically different from those reported for [^18^F]FMISO on the same cell lines (700-1500 ppm).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoroetanidazole%20AND%20rodentia%5BMeSH%5D)]

In a reported study (2) using mice bearing MCF-7, RIF-1, EMT6, HT1080/26.6, and HT1080/1-3C tumors, the normal tissue retention of [^18^F]FETA at 60 min after injection (1.48-3.7 MBq; 40-100 µCi) was found to be low (<5% injected dose (ID)/g) in lung, heart, brain, and bone. It was intermediate (5-8% ID/ g) in plasma, liver, spleen, small intestines, and muscle; and high (>8% ID/g) in kidney, bile, and urine. Significant accumulation was found in tumors (6-10% ID/g), suggesting the possibility of achieving high tumor-to-background contrast for a variety of tumors such as breast, lung, brain, and head and neck tumors.

[^18^F]FETA was found to be stable in plasma (about 93% as a parent compound at 60 min after injection) and also excreted mainly as the unchanged drug in urine (74% at 60 min after injection). In the liver, it was metabolized to catabolites that appeared to be eliminated predominantly via the hepatobiliary route.

For all of the tumor models used by Barthel et al. (2), the relative [^18^F]FETA retention, expressed as tumor-to-muscle ratio, was found to be positively correlated with the relative frequency of pO_2_ values <5 mm Hg; this correlation appeared to be linear (y = 0.04x − 1.5; r = 0.805) and significant (P = 0.027).

The biodistribution of [^18^F]FETA was assessed ex vivo and compared with [^18^F]FMISO at 2 and 4 h after intraperitoneal injections of the tracers (300 µCi/ml, 10 µl/g body mass) in C3H mice bearing KHTn tumors (1). Results showed that, at 4 h after injection, the uptakes in the heart, intestine, kidney, and tumor did not show significant differences between the two tracers but were significantly lower in the liver and lung for [^18^F]FETA.

The brain-to-blood ratio of [^18^F]FETA was found to be 1.07 ± 0.31 at 4 h after injection, showing the ability of the tracer to readily cross the normal blood-brain barrier. High-performance liquid chromatography of urine demonstrated that 10% and 15% of [^18^F]FETA -derived activity was in metabolites at 2 and 4 h after injection, respectively. In comparison, 36% and 57% of [^18^F]FMISO activity appeared as metabolites at 2 and 4 h after injection, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Fluoroetanidazole%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Fluoroetanidazole%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Fluoroetanidazole%20AND%20human)]

No publication is currently available.

## References

1 Rasey JS, Hofstrand PD, Chin LK, Tewson TJ. (1999). Characterization of [18F]fluoroetanidazole, a new radiopharmaceutical for detecting tumor hypoxia. J Nucl Med.
2 Barthel H, Wilson H, Collingridge DR, Brown G, Osman S, Luthra SK, Brady F, Workman P, Price PM, Aboagye EO. (2004). In vivo evaluation of [18F]fluoroetanidazole as a new marker for imaging tumour hypoxia with positron emission tomography. Br J Cancer.
3 Nunn A, Linder K, Strauss HW. (1995). Nitroimidazoles and imaging hypoxia. Eur J Nucl Med.
4 Hodgkiss RJ. (1998). Use of 2-nitroimidazoles as bioreductive markers for tumour hypoxia. Anticancer Drug Des.
5 Tewson TJ. (1997). Synthesis of [18F]fluoroetanidazole: a potential new tracer for imaging hypoxia. Nucl Med Biol.
6 Edwards DI. (1993). Nitroimidazole drugs--action and resistance mechanisms. I. Mechanisms of action. J Antimicrob Chemother.
7 Gamper HB, Reed MW, Cox T, Virosco JS, Adams AD, Gall AA, Scholler JK, Meyer RB. (1993). Facile preparation of nuclease resistant 3' modified oligodeoxynucleotides. Nucleic Acids Res.
8 Workman P, Brown JM. (1981). Structure-pharmacokinetic relationships for misonidazole analogues in mice. Cancer Chemother Pharmacol.